# 9-(4-[^18^F]Fluoro-3-hydroxymethylbutyl)guanine

Chemical name: | 9-(4-[^18^F]Fluoro-3-hydroxymethylbutyl)guanine
Abbreviated name: | [^18^F]FHBG
Synonym: | 2-amino-9-[3-([^18^F]fluoromethyl)-4-hydroxy-butyl]-1,9-dihydropurin-6-one
Agent category: | Compound
Target: | Herpes simplex virus thymidine kinase (HSV-TK)
Target category: | Phosphorylation
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D)]

A potential approach to the treatment of diseases and genetic disorders in humans is gene therapy [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22gene%20therapy%22%5BMeSH%20Terms%5D%20OR%20Gene%20Therapy%5BText%20Word%5D)]. This is a technique whereby the absent or malfunctioning gene is replaced by a working gene to produce an enzyme or a protein to correct the progression of disease. Noninvasive molecular imaging technologies play an important role in the fields of gene therapy by monitoring gene expression continuously in living animals (1). Magnetic resonance imaging (MRI), optical imaging, ultrasound imaging, and radionuclide imaging (positon emission tomography (PET)/single photon emission computed tomography (SPECT)) modalities have been applied for gene therapy of cancer, cardiovascular, neurological, musculoskeletal, hepatic, immunological, diabetic, and inherited diseases in small animals (2-10). These noninvasive imaging technologies allow quantitative assessments of the magnitude, location, and duration of the transgene expression.

Gene therapy can be achieved either by ex vivo or in vivo methods. The gene can be delivered using a viral or nonviral vector, such as liposome and naked DNA. Retrovirus, adenovirus, adeno-associated virus, and herpes simplex virus have been used as gene transfer vectors. Imaging transgene expression can help to optimize gene therapy. There are two imaging strategies, direct and indirect. Direct imaging uses a target-specific probe directly to the target. Indirect imaging involves coupling the target gene to a reporter gene, the gene expression of which can be tracked by a specific reporter gene probe. Currently, there are two approaches to image transgene expression, either by reporter enzyme using substrate probe or reporter receptor using receptor ligand probe. The enzymes include cytosine deaminase, β-galactosidase, tyrosinase, and herpes simplex virus type 1 thymidine kinase (HSV1-tk) or its mutant, HSV1-sr36tk. The most extensively studied reporter enzyme gene is HSV1-tk (8, 11). The reporter receptors are dopamine D_2_ receptor (D_2_R) (12) and somatostatin receptor subtype 2 (hSSTR2) (13).

HSV1-tk is a commonly studied suicide gene for cancer therapy of glioma, prostate cancer, leukemia, and lymphoma (10, 14). Suicide gene therapy is based on the enzymatic conversion of a nontoxic prodrug into a lethal drug by a transgene. Anti-HSV nucleoside analogs, such as acyclovir, ganciclovir, and penciclovir, are converted to monophosphates by HSV thymidine kinase. The cellular enzymes converted the monophosphates to di- and triphosphates, which inhibit mammalian DNA polymerase. HSV1-tk has also been widely studied as a reporter gene. The HSV prodrugs have been explored for HSV1-tk reporter gene imaging. The selective phosphorylation of the prodrug probes by HSV1-tk leads to trapping within the transduced cells and not significantly in the other cells. Many radiolabeled acycloguanosine and thymidine derivatives have been studied for HSV1-tk reporter gene imaging in vitro, in small animals, and in humans (15).

[^18^F]FHBG is a side-chain ^18^F-labeled analog of penciclovir. [^18^F]FHBG has been evaluated in vitro and in small animals and is a potential imaging agent for gene expression using PET. Noninvasive molecular imaging of therapeutic HSV1-sr36tk suicide gene therapy in mice was demonstrated with [^18^F]FHBG and [^18^F]fluorodeoxyglucose PET imaging (14). Coexpression of the reporter gene HSV1-tk and a therapeutic gene is opening up further opportunities for gene therapy (15).

### Related Resource Links:

- Chapters in MICAD (HSV-TK (http://www.ncbi.nlm.nih.gov/books/?term=HSV-TK+AND+micad%5Bbook%5D))
- Gene information in NCBI (HSV-TK (http://www.ncbi.nlm.nih.gov/gene/2703374))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

9-(4-Hydroxy-3-hydroxymethylbutyl)-guanine (penciclovir) was converted to a methoxytrityl derivative followed by tosylation. The tosylate was reacted with either tetrabutylammonium [^18^F]fluoride or [^18^F]KF in the presence of kryptofix 2.2.2, followed by acidic hydrolysis to produce 9-(4-[^18^F]fluoro-3-hydroxymethylbutyl)guanine ([^18^F]FHBG). [^18^F]FHBG was isolated by high-performance liquid chromatography (HPLC) purification. The radiochemical yield was 8.0-22.3%, with an average of 12% (corrected for decay). Synthesis time was 90-100 min, including HPLC purification with radiochemical purity >99% and average specific activity of 11.8 GBq/mmol (320 mCi/mmol) (16). Similar syntheses were later reported by others (17, 18). One-pot and automated syntheses were achieved to provide 10-15% yield in about 60 min (17, 19).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D%20AND%20in%20vitro)]

[^18^F]FHBG was shown to accumulate in HSV1-tk expressing cells in cultures. HT-29 human colon cancer cells were infected with HSV1-tk (20). In vitro uptakes of [^18^F]FHBG in the transduced cells were 31 and 71 times higher than the nontransduced cells at 1 and 5 h, respectively. HPLC analysis showed 10% intact [^18^F]FHBG, 6% monophosphate, 54% diphosphate and 30% triphosphate in the transduced cells at 5 h.

H9c2 rat embryonic cardiac cells were infected with Ad4tk, an adenovirus expression a mutant HSV1-sr39tk and vascular endothelial growth factor (VEGF_121_) independently (21). Northern blot analysis showed increasing HSV1-sr39tk and VEGF RNA expression in the transduced cells. Accumulation of [^18^F]FHBG and [^14^C]FIAU increased with increasing HSV1-sr39tk and HSV1-tk expression, respectively. Secretion of VEGF also increased with the reporter gene expressions. There is also a significant correlation of reporter gene probe uptake with VEGF production in vitro. Therefore, it may be feasible in future for monitoring angiogenesis gene therapy in vivo.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D%20AND%20rodentia)]

Tissue accumulation of [^18^F]FHBG was studied in nude mice transplanted with HT-29 human colon cancer cells with or without HSV1-tk transduction at 2 and 5 h after injection of the tracer (20). Tumor uptake of [^18^F]FHBG was 4-fold (P = 0.05) and 13-fold (P = 0.001) higher at 2 and 5 h, respectively, in tumors grown from transduced cells compared with control cells in individual animals. Bone was the only normal organ, with a high tracer uptake indicating defluorination. Transduced tumor/bone ratio of 2 stayed the same at 2 and 5 h. Transduced tumor/other normal tissue ratios were ranging from 5 to 25 at 2 h and 6 to 22 at 5 h. [^18^F]FHBG was cleared rapidly from the blood with a biphasic decrease. About 0.04%ID/g was observed in the blood at 2 h.

Rats were percutaneously injected with similar titers of adenovirus expressing HSV1-tk, HSV1-sr39tk, or control gene into the myocardium, followed by [^124^I]FIAU (HSV1-tk rats and controls) or [^18^F]FHBG (HSV1-sr39tk rats and controls) 2 days later (22). Dynamic PET was performed during the 2 h after injection of the tracer. A significant cardiac [^124^I]FIAU accumulation of a 1.24-fold increase over the controls occurred in images obtained early (10-30 min) after the tracer injection. However, no difference between HSV1-tk-infected animals and controls was seen in the images obtained later because of tracer washout. For [^18^F]FHBG, specific myocardial accumulation greater than background levels was detected in HSV1-sr39tk-infected animals at early imaging and increased over time until the latest imaging (105-120 min). At maximum, cardiac [^18^F]FHBG uptake showed a 4.15-fold increase compared with controls (105-120 min).

In another study, RG2 rat glioma tumor cells were transduced with HSV1-tk and transplanted subcutaneously in nude rats. The in vitro and in vivo imaging results show that [^124^I]FIAU is a better reporter probe than [^18^F]FHBG for imaging HSV1-tk expression, with greater sensitivity and higher accumulation at 2 h and 24 h (23). Therefore, different cell types may handle reporter gene and reporter probe differently.

Wu et al. (24) observed that the expression of two genes (HSV1-sr39tk and VEGF_121_) linked together had good correlations in cell assays in vitro and in rat infarcted myocardium imaging with [^18^F]FHBG PET. The VEGF level in the myocardial tissue was confirmed by ex vivo measurements The induced VEGF expression did not improve myocardial contractility by echocardiography, perfusion by [^13^N]ammonia imaging, and metabolism by [^18^F]fluorodeoxyglucose imaging. However, new growth of capillaries and small blood vessels was observed in the VEGF-expressing hearts. This demonstrated the feasibility of molecular imaging for monitoring angiogenic gene expression with PET reporter genes and probes.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Pigs were injected with similar titers of adenovirus expressing HSV1-sr39tk or control gene into the exposed myocardium, followed by [^18^F]FHBG 2 days later. Dynamic PET was performed during the 2 h after injection of the tracer. There was a continuous increase of [^18^F]FHBG uptake in areas infected with HSV1-sr39tk. At maximum, cardiac uptake was 2.64-fold greater than the control. About 19% of intact [^18^F]FHBG remained in the plasma at 2 h, as measured by HPLC. Only one metabolite was detected and remained unknown (22).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FHBG%5BAll%20Fields%5D%20AND%20monkeys%5BText%20Word%5D%29)]

Sequential, whole-body PET scans of two normal, cynomolgus monkeys were obtained over a period of 2 h after intravenous injection of 23-28 MBq/kg (0.62-0.76 mCi/kg) of [^18^F]FHBG. Low uptake in bone was observed in the monkeys as compared with high bone uptake in the mice. The tracer was cleared rapidly in the monkeys. In the urine, 97% of recovered activity was intact [^18^F]FHBG as compared to 69% in the plasma at 2 h after injection of the tracer (20).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fhbg%5BAll%20Fields%5D%20AND%20human)]

Human dosimetry was estimated in eight healthy volunteers by intravenous injection of 69-228 MBq (1.86-6.16 mCi) of [^18^F]FHBG (25). The average effective dose is 0.0159 mSv/MBq (58.8 mrem/mCi). The organs receiving the highest absorbed doses were the urinary bladder (0.0942 mGy/MBq or 0.349 rad/mCi), kidneys (0.0511 mGy/MBq or 0.189 rad/mCi), gut (0.0457 mGy/MBq or 0.169 rad/mCi), and liver (0.0223 mGy/MBq or 0.0825 rad/mCi). In the urine, 83% of the total activity was intact [^18^F]FHBG.

## References

1 Gambhir S.S., Herschman H.R., Cherry S.R., Barrio J.R., Satyamurthy N., Toyokuni T., Phelps M.E., Larson S.M., Balatoni J., Finn R., Sadelain M., Tjuvajev J., Blasberg R. (2000). Imaging transgene expression with radionuclide imaging technologies. Neoplasia.
2 Herschman H.R. (2004). PET reporter genes for noninvasive imaging of gene therapy, cell tracking and transgenic analysis. Crit Rev Oncol Hematol.
3 Hildebrandt I.J., Gambhir S.S. (2004). Molecular imaging applications for immunology. Clin Immunol.
4 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
5 Min J.J., Gambhir S.S. (2004). Gene therapy progress and prospects: noninvasive imaging of gene therapy in living subjects. Gene Ther.
6 Prieto J., Qian C., Hernandez-Alcoceba R., Gonzalez-Aseguinolaza G., Mazzolini G., Sangro B., Kramer M.G. (2004). Gene therapy of liver diseases. Expert Opin Biol Ther.
7 Shah K., Jacobs A., Breakefield X.O., Weissleder R. (2004). Molecular imaging of gene therapy for cancer. Gene Ther.
8 Tjuvajev J.G., Stockhammer G., Desai R., Uehara H., Watanabe K., Gansbacher B., Blasberg R.G. (1995). Imaging the expression of transfected genes in vivo. Cancer Res.
9 Wu J.C., Tseng J.R., Gambhir S.S. (2004). Molecular imaging of cardiovascular gene products. J Nucl Cardiol.
10 Yechoor V., Chan L. (2005). Gene therapy progress and prospects: gene therapy for diabetes mellitus. Gene Ther.
11 Gambhir S.S., Barrio J.R., Wu L., Iyer M., Namavari M., Satyamurthy N., Bauer E., Parrish C., MacLaren D.C., Borghei A.R., Green L.A., Sharfstein S., Berk A.J., Cherry S.R., Phelps M.E., Herschman H.R. (1998). Imaging of adenoviral-directed herpes simplex virus type 1 thymidine kinase reporter gene expression in mice with radiolabeled ganciclovir. J Nucl Med.
12 MacLaren D.C., Gambhir S.S., Satyamurthy N., Barrio J.R., Sharfstein S., Toyokuni T., Wu L., Berk A.J., Cherry S.R., Phelps M.E., Herschman H.R. (1999). Repetitive, non-invasive imaging of the dopamine D2 receptor as a reporter gene in living animals. Gene Ther.
13 Zinn K.R., Buchsbaum D.J., Chaudhuri T.R., Mountz J.M., Grizzle W.E., Rogers B.E. (2000). Noninvasive monitoring of gene transfer using a reporter receptor imaged with a high-affinity peptide radiolabeled with 99mTc or 188Re. J Nucl Med.
14 Yaghoubi S.S., Barrio J.R., Namavari M., Satyamurthy N., Phelps M.E., Herschman H.R., Gambhir S.S. (2005). Imaging progress of herpes simplex virus type 1 thymidine kinase suicide gene therapy in living subjects with positron emission tomography. Cancer Gene Ther.
15 Gambhir S.S., Barrio J.R., Herschman H.R., Phelps M.E. (1999). Imaging gene expression: principles and assays. J Nucl Cardiol.
16 Alauddin M.M., Conti P.S. (1998). Synthesis and preliminary evaluation of 9-(4-[18F]-fluoro-3-hydroxymethylbutyl)guanine ([18F]FHBG): a new potential imaging agent for viral infection and gene therapy using PET. Nucl Med Biol.
17 Penuelas I., Boan J.F., Marti-Climent J.M., Barajas M.A., Narvaiza I., Satyamurthy N., Barrio J.R., Richter J.A. (2002). A fully automated one pot synthesis of 9-(4-[18F]fluoro-3-hydroxymethylbutyl) guanine for gene therapy studies. Mol Imaging Biol.
18 Wang J.Q., Zheng Q.H., Fei X., Mock B.H., Hutchins G.D. (2003). Novel radiosynthesis of PET HSV-tk gene reporter probes [18F]FHPG and [18F]FHBG employing dual Sep-Pak SPE techniques. Bioorg Med Chem Lett.
19 Shiue G.G., Shiue C.Y., Lee R.L., MacDonald D., Hustinx R., Eck S.L., Alavi A.A. (2001). A simplified one-pot synthesis of 9-[(3-[18F]fluoro-1-hydroxy-2-propoxy)methyl]guanine([18F]FHPG) and 9-(4-[18F]fluoro-3-hydroxymethylbutyl)guanine ([18F]FHBG) for gene therapy. Nucl Med Biol.
20 Alauddin M.M., Shahinian A., Gordon E.M., Bading J.R., Conti P.S. (2001). Preclinical evaluation of the penciclovir analog 9-(4-[(18)F]fluoro-3-hydroxymethylbutyl)guanine for in vivo measurement of suicide gene expression with PET. J Nucl Med.
21 Anton M., Wittermann C., Haubner R., Simoes M., Reder S., Essien B., Wagner B., Henke J., Erhardt W., Noll S., Hackett N.R., Crystal R.G., Schwaiger M., Gansbacher B., Bengel F.M. (2004). Coexpression of herpesviral thymidine kinase reporter gene and VEGF gene for noninvasive monitoring of therapeutic gene transfer: an in vitro evaluation. J Nucl Med.
22 Miyagawa M., Anton M., Haubner R., Simoes M.V., Stadele C., Erhardt W., Reder S., Lehner T., Wagner B., Noll S., Noll B., Grote M., Gambhir S.S., Gansbacher B., Schwaiger M., Bengel F.M. (2004). PET of cardiac transgene expression: comparison of 2 approaches based on herpesviral thymidine kinase reporter gene. J Nucl Med.
23 Tjuvajev J.G., Doubrovin M., Akhurst T., Cai S., Balatoni J., Alauddin M.M., Finn R., Bornmann W., Thaler H., Conti P.S., Blasberg R.G. (2002). Comparison of radiolabeled nucleoside probes (FIAU, FHBG, and FHPG) for PET imaging of HSV1-tk gene expression. J Nucl Med.
24 Wu J.C., Chen I.Y., Wang Y., Tseng J.R., Chhabra A., Salek M., Min J.J., Fishbein M.C., Crystal R., Gambhir S.S. (2004). Molecular imaging of the kinetics of vascular endothelial growth factor gene expression in ischemic myocardium. Circulation.
25 Yaghoubi S., Barrio J.R., Dahlbom M., Iyer M., Namavari M., Satyamurthy N., Goldman R., Herschman H.R., Phelps M.E., Gambhir S.S. (2001). Human pharmacokinetic and dosimetry studies of [(18)F]FHBG: a reporter probe for imaging herpes simplex virus type-1 thymidine kinase reporter gene expression. J Nucl Med.